# 2-(4-Bromo-2,5-dimethoxyphenyl)-N-(2-[^11^C]methoxybenzyl)ethanamine

Chemical name: | 2-(4-Bromo-2,5-dimethoxyphenyl)-N-(2-[^11^C]methoxybenzyl)ethanamine
Abbreviated name: | [^11^C]CIMBI-36
Synonym:
Agent category: | Compound
Target: | 5-HT_2A_ serotonin receptor
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[P ubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-36)]

Serotonin (5-hydroxytryptamine, 5-HT) has diverse physiological roles as a neurotransmitter in the central nervous system (1). It is involved in the regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, obsessive-compulsive disorder, and schizophrenia (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are three receptor subtypes within the G-protein–coupled 5-HT_2_ receptor family: 5-HT_2A_, 5-HT_2B_, and 5-HT_2C_.

5-HT_2A_ receptors are abundantly present in the cerebral cortex, basal forebrain, hippocampus, amygdala, dorsal thalamus, hypothalamus, superior colliculus, substantia nigra, pedunculopontine nucleus, legmental area, and myelencephalon (5). 5-HT_2A_ receptors are involved in mediation of normal and psychotic states, working memory, regulation of GABAergic and cholinergic neuronal cells, sleep, peripheral pain, and cardiovascular functions. 5-HT_2B_ receptors are found mainly in several peripheral tissues, such as the stomach, intestine, pulmonary smooth muscle, and myocardium. In the brain, 5-HT_2B_ receptors are found in discrete nuclei of the cerebellum, lateral septum, dorsal hypothalamus, dorsal raphe, and amygdala. 5-HT_2C_ receptors are found in the choroid plexus, substantia nigra, globus pallidus, and ventromedial thalamus. 5-HT_2A_ receptors are implicated in several psychiatric disorders, such as schizophrenia, depression, and obsessive-compulsive disorder. Thus, there is a need for selective ligands to investigate the pharmacological role of 5-HT_2A_ receptors.

There have been several studies to develop specific 5-HT_2A_ radioligands, such as [^11^C]ketanserin (6), [^18^F]spiperone (7), [^11^C]methylspiperone ([^11^C]NMSP), and [^18^F]setoperone [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-setoperone%5BAll%20Fields%5D)], for positron emission tomography (8) imaging. However, none of these ligands has proven to be specific for 5-HT_2A_ receptors because these compounds also bind to other receptors, such as dopamine receptors and the 5-HT_1_ receptor subtypes. Altanserin, a fluorobenzoyl derivative related to ketanserin, was reported to be a potent antagonist of 5-HT_2A_ receptors with >100-fold selectivity over D_2/3_ receptors, 5-HT_1A_, 5-HT_6_, and 5-HT_7_ (9, 10). This led to the development of 3-{2-[4-(4-[^18^F]fluorobenzoyl)-1-piperidyl]ethyl}-2-sulfanyl-3H-quinazolin-4-one ([^18^F]altanserin (http://www.ncbi.nlm.nih.gov/books/NBK23366/)) as a useful tool for 5-HT_2A_ receptor PET imaging in vivo (11). 5-HT_2A_ antagonists bind to the total pool of receptors, whereas 5-HT_2A_ agonists bind only to the high-affinity functional state of the receptor but may be more important in disease states because the high affinity sites are the ones that transmit the intracellular signals. Furthermore, 2-(4-Iodo-2,5-dimethoxyphenyl)-N-(2-[^11^C]methoxybenzyl)ethanamine ([^11^C]CIMBI-5), a potent and selective 5-HT_2A_ agonist, has been shown to have similar cortical binding potentials as compared with [^18^F]altanserin in the pigs using the simplified reference tissue model (12). 2-(4-Bromo-2,5-dimethoxyphenyl)-N-(2-[^11^C]methoxybenzyl)ethanamine ([^11^C]CIMBI-36), a bromo analog of [^11^C]CIMBI-5, has also been developed as a tool for studying 5-HT_2A_ agonist binding in the brain (13).

### Related Resource Links:

- Chapters in MICAD (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=5-HT2A+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/gene/3356))
- Articles in Online Mendelian Inheritance in Man (OMIM) (5-HT_2A_ (http://www.ncbi.nlm.nih.gov/omim/182135))
- Clinical trials (5-HT_2A_ (http://www.clinicaltrials.gov/ct2/results?term=5-HT2A))
- Drug information in Food and Drug Administration (5-HT_2A_ (http://google2.fda.gov/search?q=5-HT2a&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-36%20and%20synthesis)]

Ettrup et al. (13) reported a two-step reaction synthesis of [^11^C]CIMBI-36 by reacting [^11^C]methyl triflate with the Boc-protected precursor, followed by acid hydrolysis. [^11^C]CIMBI-36 was purified with column chromatography. Specific activity was ~210 GBq/μmol (5.7 Ci/μmol) at the time of injection with a radiochemical purity >95%. The total synthesis time was 40–50 min. The lipophilicity (cLogD_7.4_) was calculated to be 3.42. The radiochemical yield was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-36%20and%20in%20vitro)]

CIMBI-36 has been reported to have high binding affinity for the 5-HT_2A_ receptor in GF62 cells transfected with 5-HT_2A_ receptors using 0.2 nM [^3^H]MDL100907 as the raioligand. Ettrup et al. (13) reported K_i_ values of 1.01 ± 0.17 and 1.7 ± 0.1 nM for 5-HT_2A_ and 5-HT_2C_, receptors, respectively. CIMBI-36 exhibited at least a 120-fold lower affinity for a variety of receptors. CIMBI-36 was found to induce phosphoinositide hydrolysis in GF62 cells with an EC_50_ of 0.53 ± 0.1 nM. These data demonstrate that CIMBI-36 is a specific and selective 5-HT_2A_ agonist.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-36%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-36%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

Ettrup et al. (13) performed PET imaging studies in two female Danish Landrace pigs with injection of ~500 MBq (13.5 mCi) [^11^C]CIMBI-36. [^11^C]CIMBI-36 exhibited high cortical accumulation, and low accumulation in the cerebellum. The two-tissue compartment distribution volume values were 13.42 and 6.76 for the frontal cortex and cerebellum, respectively. Kinetic modeling with the simplified reference tissue model (SRTM) showed that the cortical nondisplaceable binding potential (BP_ND_) values were 0.70 and 0.82 (n = 2); this value (0.70) decreased to 0.26 with ketanserin pretreatment (n = 1). As a comparison, [^11^C]CIMBI-5 and [^18^F]altanserin showed cortical SRTM BP_ND_ values of 0.46 and 0.47 (12), respectively. [^11^C]CIMBI-36 was >90% intact in the frontal cortex at 20 min after injection and ~20% intact in the plasma with two less lipophilic metabolites.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-36%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=CIMBI-36%20and%20human)]

No publication is currently available.

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Leysen J.E. (2004). 5-HT2 receptors. Curr Drug Targets CNS Neurol Disord.
6 Dewey S.L., Smith G.S., Logan J., Brodie J.D. (1993). Modulation of central cholinergic activity by GABA and serotonin: PET studies with 11C-benztropine in primates. Neuropsychopharmacology.
7 Shiue C.Y., Fowler J.S., Wolf A.P., Watanabe M., Arnett C.D. (1985). Syntheses and specific activity determinations of no-carrier-added (NCA) F-18-labeled butyrophenone neuroleptics--benperidol, haloperidol, spiroperidol, and pipamperone. J Nucl Med.
8 Gao X., Yang L., Petros J.A., Marshall F.F., Simons J.W., Nie S. (2005). In vivo molecular and cellular imaging with quantum dots. Curr Opin Biotechnol.
9 Leysen, J., Use of 5-HT receptor agonists and antagonists for the characterization of their respective recptor sites. In: A.B. Boulton, G.B. Baker and A.V. Jurio Editors, Drugs as Tools in Neurotransmitter Research. Neuromethods The Human Press, Clifton, NJ 1989: p. 299-341.
10 Tan P.Z., Baldwin R.M., Van Dyck C.H., Al-Tikriti M., Roth B., Khan N., Charney D.S., Innis R.B. (1999). Characterization of radioactive metabolites of 5-HT2A receptor PET ligand [18F]altanserin in human and rodent. Nucl Med Biol.
11 Lemaire C., Cantineau R., Guillaume M., Plenevaux A., Christiaens L. (1991). Fluorine-18-altanserin: a radioligand for the study of serotonin receptors with PET: radiolabeling and in vivo biologic behavior in rats. J Nucl Med.
12 Ettrup A., Palner M., Gillings N., Santini M.A., Hansen M., Kornum B.R., Rasmussen L.K., Nagren K., Madsen J., Begtrup M., Knudsen G.M. (2010). Radiosynthesis and evaluation of 11C-CIMBI-5 as a 5-HT2A receptor agonist radioligand for PET. J Nucl Med.
13 Ettrup A., Hansen M., Santini M.A., Paine J., Gillings N., Palner M., Lehel S., Herth M.M., Madsen J., Kristensen J., Begtrup M., Knudsen G.M. (2011). Radiosynthesis and in vivo evaluation of a series of substituted (11)C-phenethylamines as 5-HT (2A) agonist PET tracers. Eur J Nucl Med Mol Imaging.